# 2-(1E,3E,5E)-5-3-(R)-1-(1-(R)-2-(R)-2-[2-(4-(Benzo[d]thiazol-2-ylamino)phenyl)\acetamido]-6-(E)-3-(pyridin-3-yl)acrylamido)hexanamido)-5-carboxypentanamido)cyclohexyl)-27-carbamoyl-1,9,13,21,25,33-hexaoxo-5,17-dioxa-2,8,14,20,26,32-hexa-azaheptatriacontan-37-yl)-1,1-dimethyl-6,8-disulfonato-1H-benzo[e]indol-2(3H)-ylid-ene)penta-1,3-dienyl)-3-ethyl-1,1-dimethyl-1H-ben-zo[e]indolium-6,8-disulfonate

Chemical name: | 2-(1E,3E,5E)-5-3-(R)-1-(1-(R)-2-(R)-2-[2-(4-(Benzo[d]thiazol-2-ylamino)phenyl)\acetamido]-6-(E)-3-(pyridin-3-yl)acrylamido)hexanamido)-5-carboxypentanamido)cyclohexyl)-27-carbamoyl-1,9,13,21,25,33-hexaoxo-5,17-dioxa-2,8,14,20,26,32-hexa-azaheptatriacontan-37-yl)-1,1-dimethyl-6,8-disulfonato-1H-benzo[e]indol-2(3H)-ylid-ene)penta-1,3-dienyl)-3-ethyl-1,1-dimethyl-1H-ben-zo[e]indolium-6,8-disulfonate
Abbreviated name: | Cy5.5-LLP2A-6
Synonym:
Agent category: | Compound
Target: | Integrin α_4_β_1_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=119631392), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=67191026) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3676) for more information about integrin α_4_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in rodents.

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (3). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_4_β_1_ integrin plays an important role in hematopoiesis of lymphocytes. On the other hand, it affects tumor growth, tumor invasiveness, and metastasis (4). The α_4_β_1_ integrin is strongly expressed on lymphoid tumor cells (5). N-[[4-[[[(2-ethylphenyl)amino]carbonyl]amino]phenyl]acetyl]-N(epsilon)-6-[(2E)-1-oxo-3-(3-pyridinyl-2-propenyl)]-L-lysyl-L-2-aminohexanedioyl-(1-amino-1-cyclohexane)carboxamide (LLP2A) was identified as a peptidomimetic ligand to bind to α_4_β_1_ integrin on human Jurkat T-lymphoid leukemia cells using “one-bead one compound” combinatorial libraries (6, 7). A benzothiazole analog, (R)-5-(R)-[2-(2-[4-(benzothiazol-2-ylamino)-phenyl]acetylamino)-6-(E)-(3-pyridin-3-yl-acryloylamino)hexanoylamino]-5-(1-carbamoylcyclo-hexylcarbamoyl)pentanoic acid (LLP2A-6), has been conjugated with Cy5.5 (Cy5.5-LLP2A-6) to study in vivo biodistribution of the tracer in tumor-bearing mice (8). Cy5.5 is a NIR fluorescence dye with absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-LLP2A-6 has been found to have high accumulation in α_4_β_1_-positive lymphoid tumor cells in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+synthesis)]

LLP2A-6 was obtained using solid-phase synthesis (8).Cy5.5-N-hydroxysuccinimide (NHS) ester was used to conjugate LLP2A-6 using solid-phase synthesis to form Cy5.5-LLP2A-6. The NHS ester of Cy5.5 reacted with the ε-amino group of the lysine. The measured mass was m/z 2,242, which was ~1 Cy5.5/LLP2A-6. The chemical purity was >99%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+and+in+vitro)]

LLP2A-6 exhibited a 50% inhibition concentration value (IC_50_) of 53 pM in a cell-based α_4_β_1_-mediated adhesion assay using Molt-4 T-cell leukemia (α_4_β_1_-positive) with a linear peptide (25 amino acids) of fibronectin (8). LLP2A showed an IC_50_ value of 37 pM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+rodentia)]

Carpenter et al. (8) performed whole-body NIR fluorescence imaging studies of Cy5.5-LLP2A-6 in nude mice bearing Molt-4 and A549 (α_4_β_1_-negative) subcutaneous xenografts. Images were obtained after injection of the tracer (10 nmol). Substantial contrasts were observed between Molt-4 tumor tissue and normal tissue from 4 h to 120 h with a maximal difference at 4 h. Negligible fluorescence uptake into A549 tumor tissue was observed at 24 and 120 h. Ex vivo imaging showed that most of the Cy5.5-LLP2A-6 NIR fluorescent signal intensity was from the Molt-4 tumor tissue and kidneys with low signal from the liver, muscle, lung, and spleen. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LLP2A+human)]

No publication is currently available.

## NIH Support

U19 CA113298, R01 GM076151

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
4 Holzmann B., Gosslar U., Bittner M. (1998). alpha 4 integrins and tumor metastasis. Curr Top Microbiol Immunol.
5 Vincent A.M., Cawley J.C., Burthem J. (1996). Integrin function in chronic lymphocytic leukemia. Blood.
6 Peng L., Liu R., Marik J., Wang X., Takada Y., Lam K.S. (2006). Combinatorial chemistry identifies high-affinity peptidomimetics against alpha4beta1 integrin for in vivo tumor imaging. Nat Chem Biol.
7 Carpenter R.D., Andrei M., Lau E.Y., Lightstone F.C., Liu R., Lam K.S., Kurth M.J. (2007). Highly potent, water soluble benzimidazole antagonist for activated alpha 4 beta 1 integrin. J Med Chem.
8 Carpenter R.D., Andrei M., Aina O.H., Lau E.Y., Lightstone F.C., Liu R., Lam K.S., Kurth M.J. (2009). Selectively targeting T- and B-cell lymphomas: a benzothiazole antagonist of alpha4beta1 integrin. J Med Chem.